# Alexa Fluor 750-Z_HER2:342_ Affibody

Chemical name: | Alexa Flour 750-Z_HER2:342_ Affibody
Abbreviated name: | Alexa750-Z_HER2:342_
Synonym:
Agent category: | Antibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Alexa Fluor 750
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa)]

Epidermal growth factor (EGF) is a 53-amino acid growth factor (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF with at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3) and HER4 (erbB-4) (2). HER1, HER3 and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non-small-cell lung, head and neck, and colon cancer (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets (11-13). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals.

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (14). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (15-19). However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on a 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (20). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <50 nM. Various radiolabeled Affibody molecules have been studied in their ability for imaging of HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A synthetic Affibody molecule His_6_-Z_HER2:342_-Cys Affibody was labeled with Alexa Fluor 750 (Alexa750) (21). Alexa750-Z_HER2:342_ has been evaluated in nude mice bearing human SKBR-3 breast adenocarcinoma tumor.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1956)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=HER2)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20synthesis)]

His_6_-Z_HER2:342_-Cys was incubated with 5 mM neutral tris(2-carboxyethyl)phosphine solution at room temperature for 20 min (21). Immediately after the reduction, thio-reactive dye Alexa Fluor 750-maleimide was added to the mixture. Alexa750-Z_HER2:342_ was purified by column chromatography with an estimated labeling efficiencies of 60-80%, assuming a 1:1 conjugation. Alexa480-Z_HER2:342_ was also prepared similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20in%20vitro)]

Lee et al. (21) performed binding experiments with Z_HER2:342_ and Z_HER2:342_-Alexa Fluor 750 using a Biacore sensor chip immobilized with extracellular domain of chimeric HER2/Fc fusion protein. The dissociation constants (K_d_ ) of Z_HER2:342_ were calculated to be 30 pM for chimeric HER2/Fc fusion protein. The K_d_ value of Z_HER2:342_-Alexa Fluor 750 was 190 pM. Hence, the binding affinity of the synthetic Affibody molecule Z_HER2:342_-Alexa Fluor 750 was ~5 folds lower than the recombinant Affibody molecule Z_HER2:342_. Binding specificity tests in vitro showed that binding of 5 nM Z_HER2:342_-Alexa480 to SKOV-3 cells expressing HER2 was receptor mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ and trastuzumab decreased binding of Z_HER2:342_-Alexa Fluor 480 by 97% and 98%, respectively. Confocal microscopy confirmed cellular internalization of both Z_HER2:342_-Alexa480 and trastuzumab-Alexa680.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20rodentia)]

Lee et al. (21) monitored biodistribution using NIR optical imaging of HER2-expressing SKBR-3 tumor xenograft mice (n = 3/group) after intravenous injection of 10 µg Alexa750-ABD-(Z_HER2:342_)_2_, 10 µg Alexa750-Z_HER2:342_, or 50 µg Alexa750-trastuzumab. Tumor fluorescence intensities were measured at 1, 8, 24, and >48 h after tracer injection. Alexa750-ABD-(Z_HER2:342_)_2_ showed high signals around the tumor and kidney area at 8 h after injection. Fluorescence signals in the tumor area peaked ~24 h (3.6 AU) and decreased gradually to background level at 72 h. The organ with the highest concentration was the kidney (3.7 AU), followed by the liver (1.3 AU), heart (0.6 AU), lung (0.5 AU) and muscle (0.3 AU). Pre-administration of ABD-(Z_HER2:342_)_2_ (1 mg/mouse) 30 min before Alexa750-ABD-(Z_HER2:342_)_2_ injection resulted in decreased uptake in the tumor. On the other hand, Alexa750-trastuzumab exhibited moderate fluorescence intensity in the tumor, which peaked at ~48 h. Alexa750-Z_HER2:342_ exhibited a high initial accumulation in the tumor with a fast washout. The tumor clearance rates (t_½_) of Alexa750-ABD-(Z_HER2:342_)_2_, Alexa750-Z_HER2:342_, and Alexa750-trastuzumab were 40.5, 5.7, and 115 h, respectively. The maximum tumor/muscle ratios were 4.5 at 48 h for the dimer, 2.5 at 4 h for monomer, and 2.5 at 48 h for the intact trastuzumab antibody.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20human)]

No publication is currently available.

## NIH support

Intramural Research Program, N01-CO-12400, N01-CO-12401

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
12 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
13 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
14 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
15 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
16 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
17 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
18 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
19 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
20 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
21 Lee S.B., Hassan M., Fisher R., Chertov O., Chernomordik V., Kramer-Marek G., Gandjbakhche A., Capala J. (2008). Affibody molecules for in vivo characterization of HER2-positive tumors by near-infrared imaging. Clin Cancer Res.